# Hyperpolarized [1-^13^C]dehydroascorbic acid

Chemical name: | Hyperpolarized [1-^13^C]dehydroascorbic acid
Abbreviated name: | [1-^13^C]DHA
Synonym:
Agent Category: | Compound
Target: | Thoredoxin reductases
Target Category: | Enzyme
Method of detection: | Magnetic resonance imaging (MRI)/magnetic resonance spectroscopy (MRS)
Source of signal / contrast: | Hyperpolarized ^13^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Hyperpolarized%2013C)]

Magnetic resonance spectroscopy (MRS) has been noninvasively used to detect small molecules in tissues in vivo (1-4). Proton (^1^H) and carbon-13 (^13^C) are the most frequently investigated MRS applications (5-7). One technique has been often used to enhance ^13^C nuclear spins with dynamic nuclear polarization (DNP), which dramatically increases sensitivities in MRS spectra of ^13^C-labeled substrates in solutions and tissues (2, 3, 8). DNP transfers high electron-spin polarization to nuclear spins via microwave irradiation. The ^13^C MRS signals from tissues are near background levels, whereas regions with hyperpolarized ^13^C-labeled substrates provide strong signals. Thus, hyperpolarized ^13^C-labeled substrates can provide >10,000-fold enhancement of the ^13^C MRS signals from the substrate and its subsequent metabolites. ^13^C-Labeled substrates must exhibit long spin-lattice relaxation time (T_1_) values, be rapidly metabolized, and produce an observable change in the chemical shift (δ) value between the substrate and its metabolite(s). ^13^C-Labeled substrates, such as [1-^13^C]pyruvate, [2-1^3^C]fructose, [^13^C]bicarbonate, α-keto[1-^13^C]isocaproate, and [1,4-^13^C_2_]fumarate have been studied using the DNP technique in tumors in preclinical studies to measure changes in metabolism in vivo through glycolysis, citric acid cycle, amino acid metabolism and fatty acid synthesis (1-3).

Vitamin C (ascorbic acid, AA) is reversibly oxidized to DHA, which is a substrate of glucose transporters GLUT1 and GLUT3 (9). Epithelial cells of the intestine, liver, and kidney transport AA directly through sodium-dependent transporters, whereas most normal tissues acquire AA through transport of DHA (10). Intracellular DHA is then converted to AA through reaction with glutathione (GSH) or GSH-dependent enzymes and through NADPH-dependent thioredoxin reductases (11). On the other hand, tumor cells have been found to lack the capacity to transport AA and to exhibit upregulation of the GSH and thioredoxin antioxidant systems, reflecting high oxidative stress in tumor cells (10). High oxidative stress has also been implicated in neurodegenerative and cardiovascular conditions (12). Bohndiek et al. (13) generated a hyperpolarized small molecule, [1-^13^C]dehydroascorbic acid ([1-^13^C]DHA), as an imaging agent of ^13^C MRS for evaluation of intracellular reduction/oxidation (redox) status in tumors and other pathological conditions. [1-^13^C]DHA has been evaluated as an intracellular redox probe using tumor cells in vitro and in vivo. Keshari et al. (14) have performed MRS imaging of redox status in normal organs and prostate tumor in mice using hyperpolarized [1-^13^C]DHA.

### Related Resource Links:

- Chapters in MICAD (Hyperpolarized ^13^C (http://www.ncbi.nlm.nih.gov/books/?term=Hyperpolarized+13C+AND+micad%5Bbook%5D+AND+table%5Btype%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books))
- Gene information in NCBI (Thioredoxin reductase 1 (http://www.ncbi.nlm.nih.gov/gene/7296), thioredoxin reductase 2 (http://www.ncbi.nlm.nih.gov/gene/10587), GLUT1 (http://www.ncbi.nlm.nih.gov/gene/6513), GLUT3 (http://www.ncbi.nlm.nih.gov/gene/6515)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (Thioredoxin reductase 1 (http://www.ncbi.nlm.nih.gov/omim/601112), thioredoxin reductase 2 (http://www.ncbi.nlm.nih.gov/omim/606448), GLUT1 (http://www.ncbi.nlm.nih.gov/omim/138140), GLUT3 (http://www.ncbi.nlm.nih.gov/omim/138170))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Hyperpolarized%2013C%20dehydroascorbic%20acid%20synthesis)]

[1-^13^C]DHA was prepared by charcoal oxidation of commercially available [1-^13^C]AA. [1-^13^C]AA 1 (2.9 mmol) was dissolved in 15 mL methanol, and then highly purified activated charcoal Norit (0.75 g) was added as a catalyst (13). The mixture was stirred vigorously for 90 minutes at room temperature, with oxygen bubbled through at 0.2 L/minute. Charcoal was removed from the product with filtration. The final product, [1-^13^C]DHA, was then lyophilized to give a yield of 70% with >99% chemical purity. [1-^13^C]DHA (8.2 ± 1.1%, n = 8) exhibited a significantly higher degree of polarization (P < 0.05) than [1-^13^C]AA (5.1 ± 0.6%, n = 6) at pH 7 at 8 s after dissolution in phosphate-buffered saline (PBS) measured at 9.4 T. The δ values for [1-^13^C]AA and [1-^13^C]DHA were 179 ppm and 175 ppm, respectively. The T_1_ values for [1-^13^C]AA and [1-^13^C]DHA were 15.9 ± 0.7 s and 20.5 ± 0.9 s, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Hyperpolarized%2013C%20dehydroascorbic%20acid%20and%20in%20vitro)]

Bohndiek et al. (13) analyzed the conversion of [1-^13^C]DHA to [1-^13^C]AA in PBS containing 1, 5, 10, 25, and 50 mM GSH. ^13^C MRS spectra were acquired at 9.4 T. The [1-^13^C]AA signal (179 ppm) reached maximal intensity within 7–16 s. Reduction of [1-^13^C]DHA to [1-^13^C]AA was observed in RPMI medium, which contains 3.3 nM GSH and other factors. The rate of conversion observed in RPMI medium and EL4 mouse lymphoma cell suspension (1 × 10^8^ cells in 2 mL) in RPMI medium were 99 ± 6 nmol/s (n = 2) and 223 ± 18 nmol/s (n = 3), respectively. On the other hand, no oxidation of [1-^13^C]AA to [1-^13^C]DHA was observed in either RPMI medium alone or in EL4 cell suspension in RPMI medium within 60 s.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Hyperpolarized%2013C%20dehydroascorbic%20acid%20and%20rodentia)]

Bohndiek et al. (13) performed in vivo MRS studies in female C57BL/6 mice (number of mice not reported) bearing subcutaneous EL4 tumors. Hyperpolarized [1-^13^C]AA or [1-^13^C]DHA (6 mmol/mouse) was injected via tail vein catheter over a period of ~6 s. ^13^C MRS spectra were acquired at 9.4 T. After injection of [1-^13^C]DHA, the signals from [1-^13^C]AA and [1-^13^C]DHA were seen at 179 ppm and 175 ppm in the tumors, respectively. The apparent rate constant for the conversion of [1-^13^C]DHA to [1-^13^C]AA was 0.020 ± 0.004 s−^1^. The ratio of the peak integrals of [1-^13^C]AA to [1-^13^C]DHA was 0.35 ± 0.08 with an average signal/noise ratio of 67 ± 20. The EL4 tumor concentration of GSH was determined to be 1,180 nmol/g. The calculated spontaneous reaction rate constant of [1-^13^C]DHA to [1-^13^C]AA with GSH was 0.0004 s−^1^ and would produce a maximum relative signal of only 0.013 for [1-^13^C]AA in the tumors. These data suggest that an enzymatic reaction is required to account for the high rate and level of [1-^13^C]AA produced from [1-^13^C]DHA observed in the tumors. On the other hand, no observable [1-^13^C]DHA signal was detected in the tumors after injection of [1-^13^C]AA.

Keshari et al. (14) performed in vivo MRS imaging (3 T) in normal mice (n = 5) and in transgenic mice (n = 4) with adenocarcinoma of the mouse prostate (TRAMP) model after injection of 17.5 mmol of hyperpolarized [1-^13^C]DHA. T2-weighted images were obtained for 25 s at the start of [1-^13^C]DHA injection. The conversion of [1-^13^C]DHA to [1-^13^C]AA was measured as a ratio of [AA]/[AA+DHA]. In normal mice, the conversions were rapid in the liver (0.41 ± 0.03) and kidney (0.25 ± 0.03), and were significantly different (P < 0.01). These ratios were similar in TRAMP mice. In tumors of TRAMP mice, the ratio was 0.23 ± 0.03 and significantly higher than that in the normal prostate (0.06 ± 0.03, P < 0.02). Hyperpolarized ^13^C MRS imaging data acquired from rat brains (n = 3) demonstrated an even faster conversion (0.51 ± 0.10) with [1-^13^C]AA localized to the brain and [1-^13^C]DHA localized to the surrounding muscle tissue. In summary, the conversions of [1-^13^C]DHA to [1-^13^C]AA were rapid in the brain, liver, kidney, and TRAMP tumor. The conversions were slow in the normal prostate and muscle.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Hyperpolarized%2013C%20dehydroascorbic%20acid%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Hyperpolarized%2013C%20dehydroascorbic%20acid%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Hyperpolarized%2013C%20dehydroascorbic%20acid%20AND%20human)]

No references are currently available.

## References

1 Gallagher F.A., Kettunen M.I., Hu D.E., Jensen P.R., Zandt R.I., Karlsson M., Gisselsson A., Nelson S.K., Witney T.H., Bohndiek S.E., Hansson G., Peitersen T., Lerche M.H., Brindle K.M. (2009). Production of hyperpolarized [1,4-13C2]malate from [1,4-13C2]fumarate is a marker of cell necrosis and treatment response in tumors. Proc Natl Acad Sci U S A.
2 Kurhanewicz J., Bok R., Nelson S.J., Vigneron D.B. (2008). Current and potential applications of clinical 13C MR spectroscopy. J Nucl Med.
3 Mansson S., Johansson E., Magnusson P., Chai C.M., Hansson G., Petersson J.S., Stahlberg F., Golman K. (2006). 13C imaging-a new diagnostic platform. Eur Radiol.
4 Gallagher F.A., Bohndiek S.E., Kettunen M.I., Lewis D.Y., Soloviev D., Brindle K.M. (2011). Hyperpolarized 13C MRI and PET: In Vivo Tumor Biochemistry. J Nucl Med.
5 Chen A.P., Tropp J., Hurd R.E., Van Criekinge M., Carvajal L.G., Xu D., Kurhanewicz J., Vigneron D.B. (2009). In vivo hyperpolarized 13C MR spectroscopic imaging with 1H decoupling. J Magn Reson.
6 Ardenkjaer-Larsen J.H., Fridlund B., Gram A., Hansson G., Hansson L., Lerche M.H., Servin R., Thaning M., Golman K. (2003). Increase in signal-to-noise ratio of > 10,000 times in liquid-state NMR. Proc Natl Acad Sci U S A.
7 Golman K., Ardenkjaer-Larsen J.H., Petersson J.S., Mansson S., Leunbach I. (2003). Molecular imaging with endogenous substances. Proc Natl Acad Sci U S A.
8 Golman K., Olsson L.E., Axelsson O., Mansson S., Karlsson M., Petersson J.S. (2003). Molecular imaging using hyperpolarized 13C. Br J Radiol.
9 Rumsey S.C., Kwon O., Xu G.W., Burant C.F., Simpson I., Levine M. (1997). Glucose transporter isoforms GLUT1 and GLUT3 transport dehydroascorbic acid. J Biol Chem.
10 Corti A., Casini A.F., Pompella A. (2010). Cellular pathways for transport and efflux of ascorbate and dehydroascorbate. Arch Biochem Biophys.
11 Linster C.L., Van Schaftingen E. (2007). Vitamin C. Biosynthesis, recycling and degradation in mammals. FEBS J.
12 Ballatori N., Krance S.M., Notenboom S., Shi S., Tieu K., Hammond C.L. (2009). Glutathione dysregulation and the etiology and progression of human diseases. Biol Chem.
13 Bohndiek S.E., Kettunen M.I., Hu D.E., Kennedy B.W., Boren J., Gallagher F.A., Brindle K.M. (2011). Hyperpolarized [1-13C]-ascorbic and dehydroascorbic acid: vitamin C as a probe for imaging redox status in vivo. J Am Chem Soc.
14 Keshari K.R., Kurhanewicz J., Bok R., Larson P.E., Vigneron D.B., Wilson D.M. (2011). Hyperpolarized 13C dehydroascorbate as an endogenous redox sensor for in vivo metabolic imaging. Proc Natl Acad Sci U S A.